# ^125^I-Labeled anti-mucin 1 bispecific antibody bsPAM4

Chemical name: | [^125^I]-Labeled anti-mucin 1 bispecific antibody bsPAM4
Abbreviated name: | [^125^I]-bsPAM4
Synonym:
Agent Category: | Antibody
Target: | Mucin 1 (MUC1)
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4&cmd=DetailsSearch)]

The majority of individuals suffering from pancreatic adenocarcinoma (PAC) do not survive for more than 1 year after diagnosis, and <1% of these patients live beyond 5 years (1). Although surgical resection of the cancer is a possible intervention for this disease, only 10%–25% of the patients are considered suitable for this treatment because, by the time that the neoplasm is detected, the malignancy has metastasized to other organs and the tumor load in the patient is too high to warrant surgery (2). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy or a combination of the two; however, these treatments are not curative because they only prolong survival and improve the quality of life of the patient (2). The detection of this invasive cancer at an early stage would facilitate proper staging of the disease so that a suitable treatment regimen can be initiated to possibly improve patient prognosis (3).

In this regard, the monoclonal antibody (mAb) PAM4, which specifically targets mucin 1 (MUC1), a glycoprotein that is overexpressed only in PAC tumors, was developed, radiolabeled with ^131^I or ^111^In, and shown to detect neoplastic tumors with scintigraphy in patients having pancreatic malignancies (4). However, intact radiolabeled antibodies are known to have limited tumor penetration due to their large size (~150 kDa) and are of limited utility to visualize cancerous lesions with different imaging modalities (primarily positron emission tomography and single-photon emission computed tomography) due to their long circulating half-life (5). To amplify the signal obtained from an imaging agent that can be used to detect malignant tumors noninvasively, investigators have developed and evaluated a variety of strategies in preclinical studies in animals, such as pretargeting the cancer lesion with a suitable mAb (or its derivative) followed by exposing the animals to an appropriate radiolabeled, small molecular weight ligand that targets the mAb or its derivative. This technique has been shown to generate higher signal/noise ratios during imaging compared to ratios obtained with a directly labeled mAb alone (6-8). Use of the pretargeting technique for the imaging and therapy of cancer has been discussed in detail elsewhere (9, 10).

Cardillo et al. developed bsPAM4 (or bsmAb), a bispecific F(ab’)_2_ mAb fragment, by cross-linking a PAM4 Fab’ fragment to a murine anti—indium-diethylenetriamine pentaacetic acid (DTPA) mAb Fab’ fragment and using the unlabeled bsPAM4 to pretarget human CaPan-1 cell xenograft PAC tumors in nude mice (4). The animals were exposed to two radiolabeled peptide haptens, ^111^In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH_2_ ([^111^In]-IMP-156) and ^99^Tc-labeled Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH_2_ ([^99m^Tc]-IMP-192), respectively, that bind specifically to the anti-indium-DTPA mAb Fab’ fragment arm of the bsmAb. To confirm the tumor-targeting specificity of bsPAM4, the biodistribution of ^125^I-labeled bsPAM4 ([^125^I]-bsPAM4) was investigated in a group of mice bearing human PAC tumors and the results are presented in this chapter (4). The biodistribution studies performed with [^111^In]-IMP-156 (11) and [^99m^Tc]-IMP-192 (12) in mice bearing human PAC tumors pretargeted with bsPAM4 are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Peptide haptens [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=peptide%20haptens&cmd=DetailsSearch)]

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bispecific+antibody) with bispecific antibodies

Application of multivalent antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=application%20of%20multivalent%20antibodies&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20synthesis&cmd=DetailsSearch)]

The synthesis methods for bsPAM4 and bispecific rituximab (bsRIT) for use as a control were described by Cardillo et al. (4). The cross-linked bsmAbs were purified with size-exclusion chromatography (SEC), and the ratio of each Fab’ fragment in the complex was determined with high-performance liquid chromatography to be 1:1. The bsmAbs were labeled with ^125^I (bsPAM4) or ^131^I (bsRIT) with the chloramine-T method to obtain [^125^I]-bsPAM4 and [^131^I]-bsRIT (4). [^125^I]-bsPAM4 and [^131^I]-bsRIT were reported to have specific activities of 488 MBq/mg (13.2 mCi/mg) and 103 MBq/mg (2.8 mCi/mg), respectively. The radiochemical purity and yield of the radioiodinated bsmAbs were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20in%20vitro&cmd=DetailsSearch)]

Both bsPAM4 and bsRIT were reported to be stable in mouse serum and showed no aggregation or degradation for at least 5 days (incubation temperature not provided) as determined with SEC (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-bsPAM4%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^125^I]-bsPAM4 was investigated in athymic nu/nu mice bearing human PAC CaPan-1 cell tumors (4). The animals (n = 5 mice/group) were coinjected with 370 kBq/150 pmol (10 μCi/150 pmol) [^125^I]-bsPAM4 or 1.3 MBq/150 pmol (35 μCi/150 pmol) [^131^I]-bsRIT and euthanized at predetermined time points varying from 4 h to 72 h postinjection (p.i.). All organs of interest, including the tumors, were removed, and the amount of radioactivity accumulated in the various tissues was determined. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g).

The amount of radioactivity in the tumor from [^125^I]-bsPAM4 was reported to be significantly higher (P = 0.0320–0.0098) than that from [^131^I]-bsRIT at all time points (4). With [^125^I]-bsPAM4, the amount of radioactivity detected in the tumor was 6.43 ± 1.50% ID/g and 5.37 ± 2.38% ID/g at 36 h and 48 h p.i., respectively, which was significantly higher than the accumulation with the ^131^I-labeled control bsmAb (0.65 ± 0.33% ID/g and 0.47 ± 0.19% ID/g, at 36 h and 48 h p.i., respectively) (P = 0.0180 and 0.0098 at the respective time points). Although the blood clearance rates of both the radioiodinated bsmAbs were for the most part very similar, the uptake of label from [^125^I]-bsPAM4 in the non-tumor tissues was significantly higher than that observed with [^131^I]-bsRIT; e.g., at 24 h p.i., uptake in the spleen was 0.66 ± 0.06% ID/g with [^125^I]-bsPAM4 versus 0.52 ± 0.02% ID/g (P = 0.0412) with [^131^I]-bsRIT, and uptake in the muscle at the same time point was 0.30 ± 0.04% ID/g for [^125^I]-bsPAM4 versus 0.19 ± 0.02% ID/g (P = 0.0169) with [^131^I]-bsRIT, etc.

From these studies, the investigators concluded that bsPAM4 was suitable to target PAC xenograft tumors in rodents and could be used for the pretargeting studies with [^111^In]-IMP-156 and [^99m^Tc]-IMP-192 (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B125I%5D-PAM4%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported by National Institutes of Health grants CA-54425 and CA92723.

## References

1 Gold D.V., Goldenberg D.M., Karacay H., Rossi E.A., Chang C.H., Cardillo T.M., McBride W.J., Sharkey R.M. (2008). A novel bispecific, trivalent antibody construct for targeting pancreatic carcinoma. Cancer Res.
2 Gold D.V., Cardillo T., Goldenberg D.M., Sharkey R.M. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
3 Gold D.V., Goggins M., Modrak D.E., Newsome G., Liu M., Shi C., Hruban R.H., Goldenberg D.M. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
4 Cardillo T.M., Karacay H., Goldenberg D.M., Yeldell D., Chang C.H., Modrak D.E., Sharkey R.M., Gold D.V. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.
5 Ahlgren S., Orlova A., Wallberg H., Hansson M., Sandstrom M., Lewsley R., Wennborg A., Abrahmsen L., Tolmachev V., Feldwisch J. (2010). Targeting of HER2-expressing tumors using 111In-ABY-025, a second-generation affibody molecule with a fundamentally reengineered scaffold. J Nucl Med.
6 Forster G.J., Santos E.B., Smith-Jones P.M., Zanzonico P., Larson S.M. (2006). Pretargeted radioimmunotherapy with a single-chain antibody/streptavidin construct and radiolabeled DOTA-biotin: strategies for reduction of the renal dose. J Nucl Med.
7 Liu G., Dou S., Pretorius P.H., Liu X., Chen L., Rusckowski M., Hnatowich D.J. (2010). Tumor pretargeting in mice using MORF conjugated CC49 antibody and radiolabeled complimentary cMORF effector. Q J Nucl Med Mol Imaging.
8 Uppal J.K., Varshney R., Hazari P.P., Chuttani K., Kaushik N.K., Mishra A.K. (2011). Biological evaluation of avidin-based tumor pretargeting with DOTA-Triazole-Biotin constructed via versatile Cu(I) catalyzed click chemistry. J Drug Target.
9 Goldenberg D.M., Sharkey R.M. (2010). Radioactive antibodies: a historical review of selective targeting and treatment of cancer. Hosp Pract (Minneap).
10 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
11 Chopra, A., 111In-labeled Ac-Phe-Lys(DTPA)-Tyr-Lys(DTPA)-NH2 (IMP-156). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., 99mTc-Ac-Lys(DTPA)-Tyr-Lys(DTPA)-Lys(thiosemicarbazonyl-glyoxyl-cysteinyl-)-NH2 (IMP-192). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.